# N^1^,N^1^-diethyl-N^4^-(7-[^125^I]iodoquinolin-4-yl)pentane-1,4-diamine

Chemical name: | N^1^,N^1^-diethyl-N^4^-(7-[^125^I]iodoquinolin-4-yl)pentane-1,4-diamine | [image]
Abbreviated name: | ^125^I IQ | [image]
Synonym: | IQ, iodoquine | [image]
Agent Category: | Compounds | [image]
Target: | Aldehyde dehydrogenase 1A1 (ALDH1) | [image]
Target Category: | Enzyme | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) and planar imaging | [image]
Source of signal / contrast: | ^125^I | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of ^125^I IQ

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=aldehyde%20dehydrogenase%201A1%20%20and%20cancer%20stem%20cells)]

N^1^,N^1^-diethyl-N^4^-(7-[^125^I]iodoquinolin-4-yl)pentane-1,4-diamine, abbreviated as ^125^I IQ, is a compound synthesized by Chin et al. for imaging cancer stem cells (CSCs) by targeting aldehyde dehydrogenase 1A1 (ALDH1) (1).

CSCs, also known as tumor-initiating cells, have been defined as a minor population of quiescent cells that possess the capacity for self-renewal, can generate heterogeneous lineages of cancer cells, and are resistant to conventional treatment (2, 3). Currently, there are two conflicting models proposed for cancer development: the "stochastic model," which proposes that all cells have an equal possibility of acquiring mutations and initiating a tumor; and the "hierarchy model," which proposes that only a distinct and small subset of cancer cells serve as CSCs and give rise to tumors (2, 4). The latter is becoming more popular in the field of tumor biology, and the focus of treatment is shifting from cytotoxic therapy that indiscriminately kills tumor cells to CSC-targeted therapy (5). A key issue to establish CSC-targeted imaging and therapy is the identification of biomarkers that can be used to identify and isolate CSCs from diverse cell populations (1, 3).

The cytosolic activity of the enzyme ALDH1 has been shown to be a reliable marker for CSCs in various types of solid tumors (6, 7). Evidence shows that tumor cells with highly expressed ALDH1 are highly tumorigenic, and the high activity of ALDH1 is associated with poor prognosis of many types of tumors. Growing evidence further suggests that ALDH1 is not only a putative stem cell marker but may actually play multiple roles that contribute to stem cell self-protection, differentiation, and self-renewal (4). Chin et al. tested the feasibility of iodoquine (IQ) to localize CSCs by targeting the high ALDH1 activity in tumors (1). IQ is structurally identical to chloroquine (6) with the exception of the halogen substitution of iodine for chlorine. CQ is known as a weak base anti-malarial drug, which accumulates within the digestive vacuoles of parasites as well as within the lysosomes of tumor cells (8). CQ is simply metabolized by the hepatic cytochrome P450 to N-desethylchloroquine and then excreted from kidneys. Recently, Graves et al. used proteomics techniques to determine that ALDH1 is a selective target for CQ (9, 10). These characteristics make CQ an attractive candidate for high-contrast tumor imaging. Chin et al. hypothesized that the structural similarity of IQ to CQ could confer the biochemical behavior and properties similar to the CQ (1). The studies by Chin et al. supported the hypothesis and suggested that IQ is a potential radiotracer for identifying CSCs with high ALDH1 expression (1).

### Related Resource Links:

Nucleotides (http://www.ncbi.nlm.nih.gov/nuccore/?term=aldehyde%20dehydrogenase%201A1) and proteins (http://www.ncbi.nlm.nih.gov/protein/?term=aldehyde%20dehydrogenase%201A1) of aldehyde dehydrogenases

Bioassays of aldehyde dehydrogenase 1A1 (http://www.ncbi.nlm.nih.gov/pcassay/?term=aldehyde%20dehydrogenase%201A1) in PubChem

Structures and relevant information (http://www.ncbi.nlm.nih.gov/pccompound/?term=chloroquine) of chloroquine and derivatives in PubChem

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21864242)]

Chin et al. first synthesized the unlabeled IQ in a single step from the commercially available 4-chloro-7-iodoquinoline in 65% yield (1). The tin precursor was then synthesized via the Stille reaction of unlabeled IQ with excess hexabutylditin in 67% yield. The tin precursor was radioiodinated with ^125^I, ^131^I, and ^123^I with no-carrier-added synthesis with average radiochemical yields of 59.5 ± 12.5% (n = 9), 58.2 ± 14.3% (n = 4), and 57.5 ± 14.8% (n = 9), respectively. The radiochemical purity was >99%. Lipophilicity measurements with an octanol-water system revealed a partition coefficient (log P) of 0.26 ± 0.04 for ^125^I IQ, which is lower than the optimal value of 2.0–3.5 as recommended for passive brain entry (1). The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21864242)]

Cell uptake of ^125^I IQ was evaluated from 0.5 h to 4 h after incubation with cells from several cell lines (L1210cpa, L1210, A549, and MG456), and the results were expressed as a percent of the incubation dose (%) (1). L1210 cyclophosphamide-resistant (cpa) leukemia/lymphoma cell line (L1210cpa) constitutively expresses a high level of ALDH1, and its parental line L1210 expresses only a low level of ALDH1. A549 lung cancer and MG456 glioblastoma cell lines are two lines presenting high ALDH1 expression. The expression levels in these cell lines were confirmed with Western blot analysis. The results showed that L1210cpa cells had uptake levels of ^125^I IQ significantly higher than the parental line L1210 at all time points (P < 0.001) (Table 1). However, blocking studies with cold IQ showed no significant difference for the cell uptake between L1210 and L1210cpa cell lines, suggesting a nonspecific uptake mechanism such as passive diffusion (data not shown). High uptake of ^125^I IQ was also observed in A549 and CD133^+^ MG456 cells at all time points (Table 1).

Table 1: Cell uptake of ^125^I IQ at various time points after incubation with cells (%).

Cell line | ALDH1 expression | 30 min | 1 h | 2 h | 4 h
L1210 cpa | high | 20.7 ± 1.4 | 21.3 ± 0.9 | 20.6 ± 0.7 | 15.7 ± 0.7
L1210 | low | 11.0 ± 0.5 | 11.0 ± 0.4 | 9.4 ± 0.3 | 7.5 ± 0.4
A549 | high | 41.5 ± 2.4 | 43.7 ± 2.6 | 51.8 ± 2.0 | 55.6 ± 2.8
CD133^+^ MG456 | high | 81.5 ± 0.9 | 88.8 ± 0.4 | 87.8 ± 2.1 | 87.0 ± 2.4

*The ALDH1 expression level was based on the Western blotting results; no quantitative data described.

In a separate experiment, Chin et al. isolated the CD133^+^ stem cell subfraction from MG456 mouse xenograft tumors and evaluated the uptake of ^125^I IQ (1). High ^125^I IQ uptake was observed in both CD133− and CD133^+^ cells (63.6 ± 4.9% versus 43.5 ± 2.8%; n = 4/group). No explanation was given for the higher uptake in CD133− than in CD133^+^ cells.

When compared with ^18^F-FDG, the cell uptake of ^125^I IQ was higher than that of ^18^F-FDG in CD133^+^ MG456 cells (1.3 ± 0.1%, 1.3 ± 0.1%, 1.7 ± 0.2%, and 1.8 ± 0.1% at 0.5, 1, 2, and 4 h, respectively for ^18^F-FDG; P < 0.001 for all time points) (1). When assayed in phosphate-buffered saline to assess uptake in the absence of glucose in the media, ^125^I IQ uptake was modestly reduced but remained significantly higher compared to ^18^F-FDG (55.0 ± 2.5% versus 13.7 ± 6.2% at 4 h; P < 0.001). For all of these cell assays, cell viability remained >95% after the radiotracer uptake incubation period.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21864242)]

Biodistribution studies were performed in C57/B6 mice (n = 5/time point) after tail vein injection of ^125^I IQ (0.74 MBq (20 μCi)) (1). Mice were euthanized at 1, 4, and 24 h after administration, and uptake in organs was expressed as a percent of injected dose per gram (% ID/g). The biodistribution results showed that the primary route of ^125^I IQ clearance was through urinary excretion. The initial uptake in the lungs, kidneys, adrenals, and liver cleared over the subsequent 24 h. The uptake in brain was initially low (0.2 ± 0.03% ID/g at 1 h; n = 5), and remained low (0.1 ± 0.01% ID/g at 24 h; n = 5).

The radiation exposure in humans for ^123^I IQ and ^131^I IQ was estimated on the basis of the tissue radioactivity from the biodistribution studies of ^125^I IQ in mice (n = 5/time point) (1). The whole-body effective dose equivalent for ^123^I IQ was estimated to be ~0.032 and ~0.039 mSv/MBq (0.11 and 0.14 rem/mCi) for males and females, respectively. For ^131^I IQ, these values were 0.67 and 0.80 mSv/MBq (2.36 and 2.81 rem/mCi) for males and females, respectively.

Whole-body single-photon emission computed tomography (SPECT) was performed at 2–4 h after intravenous injection of ~1.85–3.7 MBq (~50–100 μCi) ^123^I IQ into mice bearing MG456 brain tumors (1). None of the small intracranial tumors (n = 4) could be visualized with SPECT imaging. Autoradiography confirmed the presence of small tumors (~1 mm in shortest diameter), and gamma counting showed overall low uptake in the entire brain specimens (0.11 ± 0.01% ID/g; n = 4). All of the large intracranial tumors (n = 3) were visualized by imaging and detected with autoradiography and histology. For large tumors that could be well excised from adjacent brain, the ^125^I IQ uptake was modest (2.3 ± 0.48% ID/g; n = 5) in a separate study (no details described).

Imaging in normal control mice (n = 4) confirmed low uptake in the brain, modest activity in the lungs and intestine, and high uptake in the genitourinary system. ^123^I IQ uptake in normal brain tissue could not be visualized. Eyes (a known site of ALDH1 expression) were visualized on all ^123^I IQ imaging studies, and this was confirmed in all subsequent mouse imaging studies with ^125^I IQ and with gamma counting of the excised eyes (2.5 ± 0.21%; n = 3 mice).

In summary, Chin et al. observed high uptake of IQ in tumor cells with high ALDH1 activity in vitro and relatively low uptake in normal brains in vivo (1). However, the uptake in the brain tumors was also low, producing relatively low contrast on images. The investigators attributed the low contrast to several possible factors, including rapid renal excretion, relatively high uptake in soft tissues such as muscle, and suboptimal SPECT imaging parameters. Although the mechanism of cellular uptake for IQ is unknown, passive diffusion with lysosomal retention is considered to be the leading putative mechanism (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

No references are currently available.

## References

1 Chin B.B., et al. (2012). Synthesis and preliminary evaluation of n.c.a. iodoquine: a novel radiotracer with high uptake in cells with high ALDH1 expression. Curr Radiopharm.
2 Rocco A., Compare D., Nardone G. (2012). Cancer stem cell hypothesis and gastric carcinogenesis: Experimental evidence and unsolved questions. World J Gastrointest Oncol.
3 Garvalov B.K., Acker T. (2011). Cancer stem cells: a new framework for the design of tumor therapies. J Mol Med (Berl).
4 Douville J., Beaulieu R., Balicki D. (2009). ALDH1 as a functional marker of cancer stem and progenitor cells. Stem Cells Dev.
5 Wu, X., H. Chen, and X. Wang, Can lung cancer stem cells be targeted for therapies? Cancer Treat Rev, 2012
6 Ginestier C., et al. (2007). ALDH1 is a marker of normal and malignant human mammary stem cells and a predictor of poor clinical outcome. Cell Stem Cell.
7 Moreb J.S. (2008). Aldehyde dehydrogenase as a marker for stem cells. Curr Stem Cell Res Ther.
8 Krafts, K., E. Hempelmann, and A. Skorska-Stania, From methylene blue to chloroquine: a brief review of the development of an antimalarial therapy. Parasitol Res, 2012
9 Graves P.R., et al. (2002). Discovery of novel targets of quinoline drugs in the human purine binding proteome. Mol Pharmacol.
10 Ma I., Allan A.L. (2011). The role of human aldehyde dehydrogenase in normal and cancer stem cells. Stem Cell Rev.